# ^99m^Tc-Labeled poly(ethyleneglycol)–N-(N-(3-diphenylphosphinopropionyl)glycyl)-S-tritylcysteine (PEG-PN_2_S)-linked ubiquicidin (UBI)

Chemical name: | ^99m^Tc-Labeled poly(ethyleneglycol)–N-(N-(3-diphenylphosphinopropionyl)glycyl)-S-tritylcysteine (PEG-PN_2_S)-linked ubiquicidin (UBI)
Abbreviated name: | [^99m^Tc]-PEG-PN_2_S-UBI_29-41_
Synonym:
Agent Category: | Peptide
Target: | Bacterial cell membrane
Target Category: | Other
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-UBI&cmd=DetailsSearch)]

Infections are the most common cause of patient morbidity in hospitals, and noninvasive imaging modalities such as X-ray/computed tomography (CT) or magnetic resonance imaging that are used to detect an infected site(s) in a patient are not able to distinguish between inflammation, tumors, and microbial infections (1). The early detection of infection in a patient can help healthcare providers devise a suitable treatment plan to control and monitor recovery from the disease. ^18^F-Labeled fluorodeoxy glucose ([^18^F]-FDG) has often been used with positron emission tomography to detect infections in the clinical setting, but the diagnosis obtained with this radiochemical must be confirmed with CT before any therapy can be initiated (2). Investigators have also used ^67^Ga-labeled citrate and ^111^In- or ^99m^Tc-labeled human immunoglobulins and monoclonal antibodies to detect infections; however, these agents show non-specific accumulation in the infected and inflamed areas of the body (3).

Researchers have shown that a thirteen-amino-acid (aa) cationic antimicrobial peptide (AMP) derived from ubiquicidin (UBI; for the aa sequence and other characteristics of UBI, see Brouwer et al. (4)) and radiolabeled directly with ^99m^Tc ([^99m^Tc]-UBI_29-41_; the aa sequence of UBI_29-41_ is: Thr-Gly-Arg-Ala-Lys-Arg-Arg-Met-Gln-Tyr-Asn-Arg-Arg) can be used to detect and distinguish infection from inflammation with scintigraphy in animals and humans (5). The mode of action of AMPs has been schematically presented and explained by Brouwer et al. (1). This labeled peptide was demonstrated to be suitable for the visualization of infections in the soft tissues, bone, bone prosthesis, and the spine (6). However, the chemical structure of the directly labeled peptides is not well understood, and the ^99m^Tc labeling of UBI_29-41_ is assumed to be due to the coordination of the radionuclide with the Lys and Arg^7^ residues in the peptide sequence as described elsewhere (7). In an effort to clearly define the chemical structure of [^99m^Tc]-UBI_29-41_, the peptide was radiolabeled with an indirect method as described by Meléndez-Alafort et al. (6). For this, UBI_29-41_ was first conjugated to a poly(ethyleneglycol) (PEG)–bearing bifunctional metal chelating agent (N-(N-(3-diphenylphosphinopropionyl)glycyl)-S-tritylcysteine (PN_2_S)) and then labeled with ^99m^Tc ([^99m^Tc]-PEG-PN_2_S-UBI_29-41_). The biodistribution and the ability of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ to visualize infection in mice with single-photon emission computed tomography (SPECT) were then compared to that of the directly labeled [^99m^Tc]-UBI_29-41_ (6).

### Related Resource Links

Ubiquicidin related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=UBI29-41+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Infection related chapters (http://www.ncbi.nlm.nih.gov/books/?term=infection+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Human antibacterial proteins (http://www.ncbi.nlm.nih.gov/protein?term=human%20antibacterial%20infection%20proteins)

Mouse (http://www.ncbi.nlm.nih.gov/protein?term=Mouse%20antibacterial%20infection%20proteins) antibacterial proteins

Antibacterial proteins in rats (http://www.ncbi.nlm.nih.gov/protein?term=Rat%20antibacterial%20proteins)

Rabbit (http://www.ncbi.nlm.nih.gov/protein?term=Rabbit%20antibacterial%20proteins) antibacterial proteins

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PEG-PN2S-UBI29-41%20synthesis&cmd=DetailsSearch)]

The synthesis of PEG-PN_2_S-UBI_29-41_ and its indirect labeling with ^99m^Tc has been described by Meléndez-Alafort et al. (6). Using the Snyder assay, the PEG-PN_2_S-UBI_29-41_ molecule was determined to be monoPEGylated (6). The radiochemical purity of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was 98 ± 1.2% (n = 20 reactions) as determined with reversed-phase high-performance liquid chromatography (RP-HPLC). The radiochemical yield and specific activity of the labeled peptide were not reported.

The direct labeling of UBI_29-41_ with ^99m^Tc was performed as described elsewhere, with a radiochemical purity of 97 ± 1.5% (n = 5 reactions) as determined with RP-HPLC (8). The radiochemical yield and specific activity of [^99m^Tc]-UBI_29-41_ were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-PEG-PN2S-UBI29-41%20in%20vitro&cmd=DetailsSearch)]

HPLC analysis showed that at least 95 ± 1% of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was intact for up to 6 h in a 1:50 dilution with 0.9% sodium chloride or 0.1 M phosphate buffer (pH 7.0) (6). When incubated with human serum, 72 ± 2.7% of the radiolabel from [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was reported to bind to high molecular weight serum proteins by 1.5 h, and the binding increased to 93 ± 1.5% after 24 h (6). The stability of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was also evaluated in different dilutions of cysteine (cysteine:[^99m^Tc]-PEG-PN_2_S-UBI_29-41_ ratios were 5:1, 50:1, and 500:1, respectively) after incubating the solutions for 1 h at 37°C (6). RP-HPLC analysis of the solutions at the end of the incubation showed that 20%, 34%, and 45% of the radioactivity was associated with cysteine in the 5:1, 50:1, and 500:1 solutions, respectively. The stability of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was not compared to that of [^99m^Tc]-UBI_29-41_ stored under the same conditions described above.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-PEG-PN2S-UBI29-41%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was compared to that of [^99m^Tc]-PEG-PN_2_S in healthy mice (n = 6 animals/group) as described by Meléndez-Alafort et al. (6). The animals (under anesthesia) were injected with the tracers through the tail vein, and SPECT images of the mice were acquired every 5 min for the next 2 h. After the imaging session, the animals were euthanized to retrieve the major organs and determine the amount of label accumulated in the various tissues. The level of radioactivity in each organ was reported as a percentage of injected dose per gram (% ID/g). Data obtained from this study showed that radioactivity from [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ accumulated primarily in organs rich in reticuloendothelial cells (e.g., liver (~40% ID/g), spleen (~25% ID/g), and lungs (~5% ID/g)) and was excreted through the urinary system. With [^99m^Tc]-PEG-PN_2_S, <5% ID/g uptake of radioactivity was observed in all of the organs. The biodistribution data obtained with [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ correlated well with the scintigraphic images obtained from animals injected with this radiochemical.

The biodistribution of [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ was also compared to that of [^99m^Tc]-UBI_29-41_ in mice (n = 6 animals/group) infected with Staphylococcus aureus in the right thigh muscle (6). The animals were injected with the radiochemicals as described above. SPECT images were obtained every 5 min for up to 2 h after injection, and the amount of label in the various tissues was determined as before. Radioactivity from [^99m^Tc]-UBI_29-41_ was present mainly in the kidneys (27.45 ± 3.81% ID/g), gall bladder (4.12 ± 0.22% ID/g), liver (1.46 ± 0.07% ID/g), and at the site of infection (2.29 ± 0.51% ID/g). All other organs showed an uptake of <0.5% ID/g tracer. With [^99m^Tc]-PEG-PN_2_S-UBI_29-41_, the label was present in the liver (14.96 ± 0.99% ID/g), kidney (14.38 ± 1.80% ID/g), spleen (6.96 ± 2.19% ID/g), gallbladder (3.52 ± 1.40% ID/g), blood (3.81 ±0.12% ID/g), lungs (2.02 ± 0.15% ID/g), and the site of infection (2.19 ± 0.40% ID/g). All other organs showed an uptake of <1.0% ID/g tracer with this radiochemical. These results indicated that [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ had a longer circulation half-life (attributed by the investigators to PEGylation (6)) than [^99m^Tc]-UBI_29-41_, which was cleared rapidly from the system. From SPECT images of the animals, it was clear that both tracers could detect the infection site in the animals as observed during the biodistribution study (6).

From these studies, the investigators concluded that, although [^99m^Tc]-PEG-PN_2_S-UBI_29-41_ can detect infections with SPECT imaging, it is not suitable for the visualization of infections in the abdomen because radioactivity from this tracer tends to accumulate in organs within the abdominal area (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-PEG-PN2S-UBI29-41%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-PEG-PN2S-UBI29-41%20Non-Human%20Primates&cmd=DetailsSearchc)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-PEG-PN2S-UBI29-41%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Brouwer C.P., Sarda-Mantel L., Meulemans A., Le Guludec D., Welling M.M. (2008). The use of technetium-99m radiolabeled human antimicrobial peptides for infection specific imaging. Mini Rev Med Chem.
2 Israel O., Keidar Z. (2011). PET/CT imaging in infectious conditions. Ann N Y Acad Sci.
3 Signore A., Mather S.J., Piaggio G., Malviya G., Dierckx R.A. (2010). Molecular imaging of inflammation/infection: nuclear medicine and optical imaging agents and methods. Chem Rev.
4 Brouwer C.P., Wulferink M., Welling M.M. (2008). The pharmacology of radiolabeled cationic antimicrobial peptides. J Pharm Sci.
5 Arteaga de Murphy C., Gemmel F., Balter J. (2010). Clinical trial of specific imaging of infections. Nucl Med Commun.
6 Melendez-Alafort L., Nadali A., Pasut G., Zangoni E., De Caro R., Cariolato L., Giron M.C., Castagliuolo I., Veronese F.M., Mazzi U. (2009). Detection of sites of infection in mice using 99mTc-labeled PN(2)S-PEG conjugated to UBI and 99mTc-UBI: a comparative biodistribution study. Nucl Med Biol.
7 Ferro-Flores G., de Maria Ramirez F., Melendez-Alafort L., de Murphy C.A., Pedraza-Lopez M. (2004). Molecular recognition and stability of 99mTc-UBI 29-41 based on experimental and semiempirical results. Appl Radiat Isot.
8 Melendez-Alafort L., Ramirez Fde M., Ferro-Flores G., Arteaga de Murphy C., Pedraza-Lopez M., Hnatowich D.J. (2003). Lys and Arg in UBI: a specific site for a stable Tc-99m complex?. Nucl Med Biol.